# ^64^Cu-4,11-Bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-Phe(4-NO_2_)-cyclo(D-Cys-Tyr-D-Trp-Lys-Thr-Cys)-D-Tyr-NH_2_

Chemical name: | ^64^Cu-4,11-Bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-Phe(4-NO_2_)-cyclo(D-Cys-Tyr-D-Trp-Lys-Thr-Cys)-D-Tyr-NH_2_
Abbreviated name: | ^64^Cu-CB-TE2A-sst_2_-ANT
Synonym:
Agent category: | Peptide
Target: | Somatostatin receptor (sst_2_)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=47117741), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=71979669) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6750) for more information about somatostatin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst2-ANT)]

Somatostatin (SST) is an inhibitor of the release of somatotropin, glucagon, insulin, gastrointestinal hormones, and other secretory proteins (1). SST is also known as somatotropin release-inhibiting factor (SRIF). SST is a cyclic polypeptide with two biologically active isoforms, SRIF-14 and SRIF-28, of 14 and 28 amino acids, respectively. SRIF has a short plasma half-life of <3 min (2). SST receptors (SSTRs) (G-protein–coupled) have been found on a variety of neuroendocrine tumors and cells of the immune system, and five individual subtypes (sst_1_–sst_5_) have been identified and subsequently cloned from animal and human tissues (3, 4). SST also inhibits cell proliferation and promotes apoptosis through binding to specific cell-surface SSTRs (5).

^111^In-Labeled diethylenetriaminepentaacetic acid-octreotide (^111^In-DTPA-OCT) is an SST analog that, over the last decade, has remained the most widely used radiopharmaceutical for the scintigraphic detection and staging of primary and metastatic neuroendocrine tumors bearing SSTRs with single-photon emission computed tomography (SPECT) (6). It has also shown promising results in peptide-receptor radionuclide therapy (7). Octreotide (OCT) is a cyclic peptide with eight amino acids. ^111^In-DTPA-OCT binds with high affinity to SSTR subtypes 2 and 5 (sst_2_ and sst_5_) and to sst_3_ to a lesser degree, but it does not bind to sst_1_ and sst_4_ (8). Currently used targeting SSTR peptides mainly are sst_2_ agonists. Therefore, there is a need for sst_2_ antagonist radioligands (9). Ginj et al. (10) have developed a series of SST antagonist ligands. One of them, Phe(4-NO_2_)-cyclo(D-Cys-Tyr-D-Trp-Lys-Thr-Cys)-D-Tyr-NH_2_ (sst_2_-ANT), was found to be a selective sst_2_ antagonist. For evaluation as a positron emission tomography (PET) imaging agent for sst_2_, ^64^Cu has been attached to sst_2_-ANT via bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane (CB-TE2A) to form ^64^Cu-CB-TE2A-sst_2_-ANT (11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst2-ANT+and+synthesis)]

CB-TE2A-sst_2_-ANT was synthesized via standard solid-phase peptide synthesis with a calculated mass of 1,479 Da in agreement with mass spectrometry (11). CB-TE2A was incorporated at the N terminus of the peptide. CB-TE2A-sst_2_-ANT was purified with high-performance liquid chromatography. ^64^Cu was complexed to CB-TE2A-sst_2_-ANT by reaction of 0.63 nmol CB-TE2A-sst_2_-ANT with 37 MBq (1 mCi) ^64^CuCl_2_ in 0.1 N HCl for 1.5 h at 95°C. ^64^Cu-CB-TE2A-sst_2_-ANT had a >95% radiochemical purity and a specific activity of 19–55 GBq/µmol (0.51–1.49 Ci/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst2-ANT+and+in+vitro)]

Wadas et al. (11) determined that ^64^Cu-CB-TE2A-sst_2_-ANT showed a K_d_ (affinity constant) of 26.0 ± 2.4 nM and a B_max_ (receptor density) of 23 pmol/mg protein in AR42J (sst_2_-positive) tumor cell homogenates. On the other hand, ^64^Cu-CB-TE2A-Y3-TATE (sst_2_-selective agonist) exhibited a K_d_ of 1.7 nM and a B_max_ of 1.6 pmol/mg protein. This is consistent with the observation that antagonists bind to all sites whereas agonists bind only to the high affinity sites. Ginj et al. (10) also reported that sst_2_-ANT had 50% inhibition concentration (IC_50_) values of >1,000, 3.6 ± 0.4, >1,000, 349 ± 30, and 276 ± 119 nM for human sst_1_, sst_2_, sst_3_, sst_4_, and sst_5_ receptors in competition with ^125^I-SRIF-28, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst2-ANT+and+rodentia)]

Wadas et al. (11) performed ex vivo biodistribution studies with ^64^Cu-CB-TE2A-sst_2_-ANT in rats (n = 3/group) bearing xenografts of AR42J tumor cells at 1, 4, and 24 h after injection. The accumulation of radioactivity in the sst_2_ tumors was 1.69% injected dose per gram (% ID/g) at 1 h, 1.81% ID/g at 4 h, and 0.84% ID/g at 24 h after injection. The adrenal was the organ that had the highest accumulation (3.46% ID/g) at 4 h after injection, followed by the kidney (2.83% ID/g), pancreas (2.56% ID/g), liver (1.32% ID/g), and pituitary (1.17% ID/g). Accumulation of radioactivity in the other tissues was low. The concentration in the blood was 0.05% ID/g at 4 h after injection, with tumor/blood ratios of 7, 35, and 72 at 1, 4, and 24 h, respectively. Co-injection with sst_2_-ANT reduced the accumulation of radioactivity by 74% in the tumors, 85% in the adrenal, 85% in the pancreas, 70% in the pituitary, and 50% in the stomach at 4 h after injection. Little or no inhibition was observed in the other tissues. The tumor/blood ratio was reduced to 6 from 35. Whole-body SPECT imaging visualized the sst_2_ tumor as early as 1 h after injection. Tumor/muscle ratios were 58 and 37 at 4 h and 24 h, respectively. Co-injection with sst_2_-ANT reduced the accumulation of radioactivity by 75% in the tumors at 4 h after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst2-ANT+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst2-ANT+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst2-ANT+and+human)]

No publication is currently available.

## NIH Support

R24 CA83060, F32 CA115148, R01 CA064475, R01 EB 1430, R24 CA86307

## References

1 Weckbecker G., Lewis I., Albert R., Schmid H.A., Hoyer D., Bruns C. (2003). Opportunities in somatostatin research: biological, chemical and therapeutic aspects. Nat Rev Drug Discov.
2 Patel Y.C., Wheatley T. (1983). In vivo and in vitro plasma disappearance and metabolism of somatostatin-28 and somatostatin-14 in the rat. Endocrinology.
3 Corleto V.D., Nasoni S., Panzuto F., Cassetta S., Delle Fave G. (2004). Somatostatin receptor subtypes: basic pharmacology and tissue distribution. Dig Liver Dis.
4 Moller L.N., Stidsen C.E., Hartmann B., Holst J.J. (2003). Somatostatin receptors. Biochim Biophys Acta.
5 Barnett P. (2003). Somatostatin and somatostatin receptor physiology. Endocrine.
6 Krenning E.P., Kwekkeboom D.J., Bakker W.H., Breeman W.A., Kooij P.P., Oei H.Y., van Hagen M., Postema P.T., de Jong M., Reubi J.C., et al. (1993). Somatostatin receptor scintigraphy with [111In-DTPA-D-Phe1]- and [123I-Tyr3]-octreotide: the Rotterdam experience with more than 1000 patients. Eur J Nucl Med.
7 Kwekkeboom D.J., Mueller-Brand J., Paganelli G., Anthony L.B., Pauwels S., Kvols L.K. (2005). M. O'Dorisio T, R. Valkema, L. Bodei, M. Chinol, H.R. Maecke, and E.P. Krenning, Overview of results of peptide receptor radionuclide therapy with 3 radiolabeled somatostatin analogs. J Nucl Med.
8 Storch D., Behe M., Walter M.A., Chen J., Powell P., Mikolajczak R., Macke H.R. (2005). Evaluation of [99mTc/EDDA/HYNIC0]octreotide derivatives compared with [111In-DOTA0,Tyr3, Thr8]octreotide and [111In-DTPA0]octreotide: does tumor or pancreas uptake correlate with the rate of internalization?. J Nucl Med.
9 Reubi J.C., Schar J.C., Waser B., Wenger S., Heppeler A., Schmitt J.S., Macke H.R. (2000). Affinity profiles for human somatostatin receptor subtypes SST1-SST5 of somatostatin radiotracers selected for scintigraphic and radiotherapeutic use. Eur J Nucl Med.
10 Ginj M., Zhang H., Waser B., Cescato R., Wild D., Wang X., Erchegyi J., Rivier J., Macke H.R., Reubi J.C. (2006). Radiolabeled somatostatin receptor antagonists are preferable to agonists for in vivo peptide receptor targeting of tumors. Proc Natl Acad Sci U S A.
11 Wadas T.J., Eiblmaier M., Zheleznyak A., Sherman C.D., Ferdani R., Liang K., Achilefu S., Anderson C.J. (2008). Preparation and biological evaluation of 64Cu-CB-TE2A-sst2-ANT, a somatostatin antagonist for PET imaging of somatostatin receptor-positive tumors. J Nucl Med.